# D-Cys-D-Asp-Gly-Leu-Gly-ProOH-Asn-D-Cys-biotin-streptavidin-Cy5.5

Chemical name: | D-Cys-D-Asp-Gly-Leu-Gly-ProOH-Asn-D-Cys-biotin-streptavidin-Cy5.5
Abbreviated name: | LXY1-biotin-SA-Cy5.5
Synonym: | cdGLGBNc-biotin-SA-Cy5.5
Agent category: | Peptide
Target: | Integrin α_3_
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=152013007), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=152013006) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3675) for more information about integrin α_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (3). They consist of an α and a β subunit, and they important for cell adhesion and signal transduction. The α_3_β_1_ integrin plays an important role in normal lung, kidney, cerebral cortical, and epithelial development (4). On the other hand, it affects tumor growth, tumor invasiveness, and metastasis as the α_3_ integrin is strongly expressed on tumor cells (5, 6). D-Cys-D-Asp-Gly-Leu-Gly-ProOH-Asn-D-Cys (LXY1), a cyclic peptide, was identified to bind to α_3_ integrin on human ovarian cancer cells using “one-bead one compound” combinatorial libraries (7, 8). LXY1 was conjugated with Cy5.5 via biotin-streptavidin (SA) to study in vivo biodistribution of the tracer in tumor-bearing mice. Cy5.5 is a NIR fluorescence dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. LXY1-Biotin-SA-Cy5.5 was found to have a high specific accumulation in α_3_-positve human glioblastoma U-87MG cells in nude mice (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+synthesis)]

LXY1 and LXY1-biotin were constructed using solid-phase synthesis (9). SA-Cy5.5 (1.8 nmol) and LXY1-biotin (7.2 nmol) were incubated for 18 h at 4°C to form LXY1-biotin-SA-Cy5.5 (molecular weight, 64 kDa) complexes with a 4:1 molar ratio of biotin/SA. LXY1-Lys(NH_2_)-CONH_2_ was incubated with Cy5.5-NHS for 18 h to form LXY1-Lys-Cy5.5 (LXY1-Cy5.5). The NHS ester of Cy5.5 was reacted with the ε-amino group of the lysine. The peak containing the LXY1-Cy5.5 conjugate (2.28 kDa) was analyzed with matrix-assisted laser desorption/ionization-time-of-flight mass spectrometry (MALDI-TOF MS) and found to be consistent with 1 Cy5.5 per LXY1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+in+vitro)]

Xiao et al. (9) showed that the binding affinity (K_d_) of LXY1-biotin for integrin α_3_ on U-87MG cells was 0.5 ± 0.1 µM. The LXY1-biotin binding to U-87MG cells was completely inhibited by excess LXY1 and anti-α_3_ antibody. Yao et al. (10) showed that LXY1 binds only to integrin α_3_ and not to other integrins tested (α_1_, α_2_, α_3_, α_5_, α_6_, α_9_, α_V_, β_1_, β_2_, β_3_, β_4_, and β_5_).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+rodentia)]

Biodistribution studies of LXY1-biotin-SA-Cy5.5 were evaluated in nude mice (n = 3/group) bearing subcutaneous U-87MG and K562 (α_3_-negatve) xenografts (9). Ex vivo images were obtained after injection of 7.2 nmol LXY1-biotin-SA-Cy5.5 at 0.5, 4, 6, 24, and 48 h after injection. The NIR fluorescence intensities of LXY1-biotin-SA-Cy5.5 in the U-87MG tumor and kidneys peaked at ~4 h and then decreased gradually, but >80% of the maximum value was retained in the tumor even at 48 h. The NIR fluorescence intensities in the liver, skin, intestine, spleen, and brain were lower than the intensities in the tumor and kidneys. Little NIR fluorescence signal was observed in the K562 tumors. Pretreatment with 3.6 μmol LXY1 or 0.13 nmol anti-α_3_ integrin antibody 1 h before administration of LXY1-biotin-SA-Cy5.5 showed that accumulation of the imaging probe in the U-87MG tumor was almost completely blocked by LXY1 (P < 0.001) and anti-α3 integrin antibody (P < 0.001). On the other hand, the pretreatments had no effect on the NIR fluorescence signals in the liver and kidneys. The smaller univalent LXY1-Cy5.5 exhibited a faster accumulation in the tumor and kidneys, and LXY1-Cy5.5 exhibited a more rapid clearance than the multivalent LXY1-biotin-SA-Cy5.5. Whole-body NIR fluorescence imaging showed that the U-87MG tumor but not the K562 tumor was clearly visualized with LXY1-biotin-SA-Cy5.5.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LXY1+and+human)]

No publication is currently available.

## NIH Support

R33 CA86364, R33 CA99136, U19 CA113298, P50 CA97257

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
4 Hynes R.O. (2002). Integrins: bidirectional, allosteric signaling machines. Cell.
5 Albelda S.M., Mette S.A., Elder D.E., Stewart R., Damjanovich L., Herlyn M., Buck C.A. (1990). Integrin distribution in malignant melanoma: association of the beta 3 subunit with tumor progression. Cancer Res.
6 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
7 Aina, O.H., R. Liu, J.L. Sutcliffe, J. Marik, C.X. Pan, and K.S. Lam, From Combinatorial Chemistry to Cancer-Targeting Peptides. Mol Pharm, 2007
8 Aina O.H., Marik J., Liu R., Lau D.H., Lam K.S. (2005). Identification of novel targeting peptides for human ovarian cancer cells using "one-bead one-compound" combinatorial libraries. Mol Cancer Ther.
9 Xiao W., Yao N., Peng L., Liu R., Lam K.S. (2009). Near-infrared optical imaging in glioblastoma xenograft with ligand-targeting alpha3 integrin. Eur J Nucl Med Mol Imaging.
10 Yao N., Xiao W., Wang X., Marik J., Park S.H., Takada Y., Lam K.S. (2009). Discovery of targeting ligands for breast cancer cells using the one-bead one-compound combinatorial method. J Med Chem.